# ^111^In-Tetrameric Plectin-1 targeting peptide (4(βAKTLLPTP-GGS(PEG5000))KKK-^111^In-DOTA-βA-NH_2_)

Chemical name: | ^111^In-Tetrameric Plectin-1 targeting peptide (4(βAKTLLPTP-GGS(PEG5000))KKK-^111^In-DOTA-βA-NH_2_)
Abbreviated name: | ^111^In-tPTP
Synonym: | ^111^In-Tetrameric Plectin-1 targeting peptide
Agent category: | Peptide
Target: | Plectin-1
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma imaging
Source of signal\contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=134044255), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=47607491) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=5339) for more information about Plectin-1.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=tPTP)]

Patients with pancreatic ductal adenocarcinoma (PDAC) have a median survival of 6 months and a 5-year survival rate of only 3% (1). PDAC is an aggressive cancer with early metastasis in >80% of patients. Early detection would be particularly useful for monitoring people at high risk of developing pancreatic cancer. Plectin-1 was identified in 100% of tested PDAC lesions and 60% of tested preinvasive PanIN III lesions (2). Plectin-1, a cytoskeletal component, is not expressed in the normal pancreas, liver, lymph node, lung, or peritoneum in humans. Using phage display screenings, the linear peptide Lys-Thr-Leu-Leu-Pro-Thr-Pro (KTLLPTP) (Plectin-1–targeting peptide, PTP) (3) has been found to specifically bind to Plectin-1 (4, 5), a protein present both inside and on the membrane of human and mouse PDAC cells but only on the inside of normal pancreatic cells. Kelly et al. (3) conjugated PTP to Cy5.5-labeled cross-linked iron oxide particles (CLIO-Cy5.5) for imaging Plectin-1 expression in PDAC, which suggests that Plectin-1 can serve as a biomarker for PDAC. Bausch et al. (2) labeled a tetrameric PTP with ^111^In (4(βAKTLLPTP-GGS(PEG5000))KKK-^111^In-DOTA-βA-NH_2_) (^111^In-tPTP) for single-photon emission computed tomography (SPECT) imaging for primary and metastatic pancreatic tumors.

### Related Resource Links:

- Chapters in MICAD (Plectin-1 (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=Plectin-1%5BAll+Fields%5D+AND+micad%5Bbook%5D))
- Gene information in NCBI (Plectin-1 (http://www.ncbi.nlm.nih.gov/gene/5339)).
- Articles in Online Mendelian Inheritance in Man (OMIM) (Plectin-1 (http://www.ncbi.nlm.nih.gov/omim/601282))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=tPTP%20and%20synthesis)]

4(βAKTLLPTP-GGS(PEG5000))KKK-DOTA-βA-NH_2_ (tPTP) (100 µg) was incubated with 185 MBq (5 mCi) ^111^InCl_3_ in ammonium acetate buffer (pH 4.5) for 15 min at 40°C (2). ^111^In-tPTP was purified with column chromatography. The yield, radiochemical purity, and specific activity of ^111^In-tPTP were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=tPTP%20and%20in%20vitro)]

Competition binding assays were performed in Plectin-1–positive L3.6pl PDAC cells using ^111^In-tPTP with tPTP. tPTP had a K_i_ value of 830 nM (2).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=tPTP%20and%20rodentia)]

Bausch et al. (2) performed ex vivo biodistribution studies in mice bearing orthotopically implanted L3.6pl (n = 10), Panc1 (n = 5), or AK134 (n = 8) PDAC tumor cells at 4 h after injection of 37 MBq (1 mCi) ^111^In-tPTP. Tumor accumulation of radioactivity was 2.0% injected dose per gram (ID/g), 1.8% ID/g, 1.5% ID/g, and 0.5% ID/g for L3.6pl, Panc1, AK134, and normal pancreas, respectively. Accumulation in these mice was highest in the kidney with 15%–22% ID/g, followed by the liver with 1.7%–2.6% ID/g. Immunohistochemistry of sections of the pancreas and peritoneum metastases confirmed the presence of Plectin-1–expressing tumor cells in the pancreas and peritoneum.

SPECT scanning clearly visualized the three tumors and the kidneys at 4 h after injection. SPECT scanning located metastases in the peritoneum of two mice, which were confirmed with autopsy. In a model of AK134 PDAC liver metastasis, SPECT/computed tomography scanning clearly identified tumor lesions in the liver, which were confirmed with autopsy.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=tPTP%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=tPTP%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=tPTP%20and%20human)]

No publication is currently available.

## NIH Support

R01 CA137071-02, R01 CA137071-04, R01 EB010023-01A1, R01 EB010023-02

## References

1 Li D., Xie K., Wolff R., Abbruzzese J.L. (2004). Pancreatic cancer. Lancet.
2 Bausch D., Thomas S., Mino-Kenudson M., Fernandez-del C.C., Bauer T.W., Williams M., Warshaw A.L., Thayer S.P., Kelly K.A. (2011). Plectin-1 as a novel biomarker for pancreatic cancer. Clin Cancer Res.
3 Kelly K.A., Bardeesy N., Anbazhagan R., Gurumurthy S., Berger J., Alencar H., Depinho R.A., Mahmood U., Weissleder R. (2008). Targeted nanoparticles for imaging incipient pancreatic ductal adenocarcinoma. PLoS Med.
4 Andra K., Kornacker I., Jorgl A., Zorer M., Spazierer D., Fuchs P., Fischer I., Wiche G. (2003). Plectin-isoform-specific rescue of hemidesmosomal defects in plectin (-/-) keratinocytes. J Invest Dermatol.
5 Sonnenberg A., Liem R.K. (2007). Plakins in development and disease. Exp Cell Res.